# ^68^Ga-N,N’-bis[2-Hydroxy-5-(carboxyethyl)benzyl]ethylenediamine-N,N’-diacetic acid-polyethylene glycol-single-chain Cys-tagged vascular endothelial growth factor-121

Chemical name: | ^68^Ga-N,N’-bis[2-Hydroxy-5-(carboxyethyl)benzyl]ethylenediamine-N,N’-diacetic-polyethylene glycol-single-chain Cys-tagged vascular endothelial growth factor-121
Abbreviated name: | ^68^Ga-HBED-CC-PEG-scVEGF
Synonym:
Agent category: | Polypeptide
Target: | Vascular endothelial growth factor receptor-2 (VEGFR-2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFRs) on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells, such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells, also express VEGFRs (1).

VEGFRs have been found to be overexpressed in various tumor cells and tumor-associated endothelial cells but are not detectable in quiescent endothelial cells (3). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). A 15-amino-acid fusion tag (Cys-tag) was developed for site-specific conjugation via the free sulfhydryl group of Cys. Backer et al. (9) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain 3–112 amino acid fragments of VEGF_121_ joining head-to-tail to express as scVEGF, which was labeled as ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-polyethylene glycol (PEG)-scVEGF (^64^Cu-DOTA-PEG-scVEGF), ^99m^Tc-hydrazinonicotinic acid (HYNIC)-scVEGF (^99m^Tc-HYNIC-scVEGF), and Cy5.5-scVEGF for imaging VEGFR expression to study tumor angiogenesis. In this chapter, ^68^Ga-N,N’-bis[2-Hydroxy-5-(carboxyethyl)benzyl]ethylenediamine-N,N’-diacetic acid-PEG-scVEGF (^68^Ga-HBED-CC-PEG-scVEGF) is being developed for positron emission tomography (PET) imaging of VEGFR-2 in tumor vasculature (10).

### Related Resource Links:

- Chapters in MICAD (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VEGFR+AND+micad%5Bbook%5D))
- Gene information in NCBI (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3791))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=VEGFR))
- Clinical trials (VEGFR (http://www.clinicaltrials.gov/ct2/results?term=VEGFR))
- Drug information in FDA (VEGFR (http://google2.fda.gov/search?q=VEGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+synthesis)]

Backer et al. (9) reported the synthesis of a Cys-tagged vector of VEGF_121_ by cloning two single-chain 3–112 amino acid fragments of VEGF_121_ joining head-to-tail to express as scVEGF in Escherichia coli for mammalian cell production. ^68^Ga labeling of scVEGF was performed through HBED-CC chelation (10). The HBED-CC group was activated by five-fold molar excess of N-hydroxysuccinimide-PEG-maleimide for 60 min (pH 8). A mixture of scVEGF and the activated HBED-CC in a molar ratio of 1:10 was incubated for 60 min. The HBED-CC-PEG-scVEGF conjugate was purified with high-performance liquid chromatography. The number of HBED-CC molecules per protein was ~1. For radiolabeling, 3 nmol HBED-CC-PEG-scVEGF was added to 30–50 MBq (0.81–1.35 mCi) ^68^Ga diluted in buffer (pH 4.2). ^68^Ga-HBED-CC-PEG-scVEGF was purified with column chromatography with a radiolabeling yield of 98.7%. ^68^Ga-HBED-CC-PEG-scVEGF was stable in phosphate-buffered saline (pH 7) for at least 4 h. Specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+and+in+vitro)]

In vitro competition binding studies were performed in 293/KDR cells expressing cloned human VEGFR-2 (10). HBED-CC-PEG-scVEGF inhibited the binding of ^68^Ga-HBED-CC-PEG-scVEGF to VEGFR-2 on the cells with a K_d_ of 0.67 ± 0.15 nM and a B_max_ of 1.1 × 10^6^ binding sites per cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+rodentia)]

Eder et al. (10) performed ex vivo biodistribution studies of ^68^Ga-HBED-CC-PEG-scVEGF in nude mice (n = 3/group) bearing HT-29 human colon adenocarcinoma tumors expressing VEGFR-2 at 1, 2, 3, and 4 h after injection. The tumor accumulated 2.07%, 1.87%, 1.56%, and 1.48% injected dose per gram (ID/g) at 1, 2, 3, and 4 h, respectively. The blood concentration levels at these time points were 5.84%, 3.20%, 1.37%, and 1.34% ID/g, respectively. The organs with the highest accumulation of ^68^Ga-HBED-CC-PEG-scVEGF at 2 h after injection were the kidneys (179% ID/g), liver (3.6% ID/g), lung (3.5% ID/g), and heart (3.4% ID/g). The tumor/blood and tumor/muscle ratios at 4 h after injection were 1.1 and 2.1, respectively. Injection of inactivated ^68^Ga-PEG-scVEGF showed ~0.8% ID/g tumor accumulation at 1 h after injection. However, no blocking studies were performed. PET imaging studies were performed at 1.5 h after injection of ^68^Ga-HBED-CC-PEG-scVEGF with good tumor/background contrast.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Itakura J., Ishiwata T., Shen B., Kornmann M., Korc M. (2000). Concomitant over-expression of vascular endothelial growth factor and its receptors in pancreatic cancer. Int J Cancer.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Backer M.V., Patel V., Jehning B.T., Claffey K.P., Backer J.M. (2006). Surface immobilization of active vascular endothelial growth factor via a cysteine-containing tag. Biomaterials.
10 Eder M., Krivoshein A.V., Backer M., Backer J.M., Haberkorn U., Eisenhut M. (2010). ScVEGF-PEG-HBED-CC and scVEGF-PEG-NOTA conjugates: comparison of easy-to-label recombinant proteins for [68Ga]PET imaging of VEGF receptors in angiogenic vasculature. Nucl Med Biol.